# ^64^Cu-Labeled NOTA-conjugated anti-CD105 (endoglin) chimeric monoclonal antibody linked to near-infrared dye IRDye 800CW

Chemical name: | ^64^Cu-Labeled NOTA-conjugated anti-CD105 (endoglin) chimeric monoclonal antibody linked to near-infrared dye IRDye 800CW
Abbreviated name: | [^64^Cu]-NOTA-TRC105-800CW
Synonym:
Agent Category: | Antibody
Target: | CD105 (endoglin) antigen
Target Category: | Antigen
Method of detection: | Multimodal (positron emission tomography (PET); optical imaging (near-infrared (NIRF) imaging)
Source of signal / contrast: | ^64^Cu (PET); IRDye 800CW (NIRF)
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=CD105&cmd=DetailsSearch)]

The CD105 antigen (endoglin) is a hypoxia-inducible, 180-kDa, disulfide-linked homodimeric transmembrane glycoprotein that is a co-receptor for the transforming growth factor β (TGF-β) (1). Both CD105 and TGF-β are expressed at low levels in resting endothelial cells, but they are overexpressed in cancerous lesions and play a significantly pro-angiogenic role in remodeling the vasculature of malignant tumors (2). It has been shown that the levels of CD105 in endothelial tissues correlate well with the degree of cell proliferation, that the antigen is a suitable biomarker to quantify tumor angiogenesis and can be used to determine the prognostic outcome for cancer patients (3). Investigators have reported that immunotoxins and radioimmunoconjugates generated with anti-CD105 monoclonal antibodies (mAbs) can inhibit angiogenesis and prevent the growth and metastasis of cancerous tumors (4). The biological activity of CD105 has been discussed by Seon et al. (4). For translation to the clinic, a human/mouse chimeric anti-CD105 mAb (designated c-SNj6 or TRC105) was generated and shown to have suitable pharmacokinetic, toxicological, and immunogenicity characteristics for use in non-human primates (5). Currently, a clinical trial (http://clinicaltrials.gov/ct2/show/NCT01326481?term=endoglin&rank=5) is in progress to evaluate the use of TRC105 for the treatment of metastatic breast cancer.

TRC105 was labeled with ^64^Cu (6) and ^89^Zr (7), respectively, and shown to detect the expression of CD105 with positron emission tomography (PET) imaging in xenograft tumors in mice. In another study, TRC105 was conjugated to IRDye 800CW, a near-infrared fluorescent (NIRF) dye, and the expression of CD105 in tumors could be visualized with NIRF imaging (8). Either PET or NIRF imaging can be used by itself for the in vivo detection of tumors, but the former has high sensitivity and can be used for whole-body scans, whereas the main drawback of this modality is that it has low spatial resolution. The latter imaging method generates fluorescence signals that can be used to visualize the target tissue in real time, but this imaging modality cannot be used for whole-body scans or for the precise quantification of the target molecule(s) (9). Therefore, the combination of PET and NIRF imaging capabilities within the same agent would greatly improve the noninvasive investigative potential of a probe at the preclinical or clinical stages because each modality will complement the deficiency of the other (10). In addition, a dual-modality PET/NIRF imaging probe can be utilized to identified to locate neoplastic tumors with a whole-body PET scan, and later NIRF imaging can be used by surgeons to visualize the lesions for surgical resection (11). On the basis of this idea, TRC105 was conjugated with 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA), a metal chelating agent, and IRDye 800CW (an NIRF dye with excitation at 778 nm and emission at 806 nm). The double-conjugated mAb was then labeled with ^64^Cu (half-life = 12.7 h), and the multimodal agent ([^64^Cu]-NOTA-TRC105-800CW) was evaluated for the PET and NIRF detection of 4T1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) cell tumors in mice (11).

### Related Resource Links

TRC105 (http://www.ncbi.nlm.nih.gov/books/?term=TRC105+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters in MICAD

Other anti-CD105 antibody chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-CD105+antibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human CD105 (endoglin) protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/BC014271.2) sequences

CD105 gene information (http://www.ncbi.nlm.nih.gov/gene/2022) (Gene ID: 2022)

CD105 in Online Mendelian Inheritance in Man Database (http://omim.org/entry/131195) (OMIM)

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=TRC105) related to TRC105

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-TRC105-800CW%20synthesis&cmd=DetailsSearch)]

TRC105 was obtained from a commercial source, and the mAb was conjugated with NOTA and IRDye 800CW, respectively, as described by Zhang et al. (11). NOTA-TRC105-800CW was purified on a PD-10 column and labeled with ^64^Cu as detailed elsewhere (11). The radiolabeled and NIRF-conjugated mAb was purified on a PD-10 column with phosphate-buffered saline (pH not reported) as the mobile phase and passed through a 0.22-μm filter for use in in vivo studies.

Cetuximab (a human/mouse chimeric mAb that targets the human epidermal growth factor receptor) was obtained from a pharmaceutical company and used to prepare [^64^Cu]-NOTA-cetuximab-800CW for use as control (11).

The total time taken to prepare the two purified ^64^Cu-labeled mAbs was reported to be 60 ± 10 min (n = 10 preparations), and both labeled mAbs had a radiochemical yield and radiochemical purity of >85% and >98%, respectively (11). The specific activity of the two ^64^Cu-labeled and 800CW-conjugated mAbs was ~1.3 GBq (35.1 mCi)/6.5 nmol (11). Ultraviolet spectrophotometric analysis revealed that on average ~5 NOTA and 0.9 800CW molecules were conjugated to each of the mAbs.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-TRC105-800CW%20in%20vitro%20studies&cmd=DetailsSearch)]

A fluorescence-assisted cell-sorting analysis of HUVEC (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1730&Template=cellBiology) cells (human umbilical vein endothelial cells that express CD105) and 4T1 cells (murine breast cancer cells that do not express CD105) with AlexaFluor488- and Cy3-labeled secondary antibodies showed that both TRC105 and NOTA-TRC105-800CW had similar affinities for the CD105 antigen (11). This indicated that conjugation of NOTA and IRDye 800CW to TRC105 did not alter its affinity or specificity for the antigen targeted on the cell surface. No blocking studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-TRC105-800CW%20rodentia&cmd=DetailsSearch)]

4T1 cells were used to generate tumors in mice because these cells do not express the CD105 antigen and angiogenesis in the tumor would be only with the endothelial cells that express this antigen. Therefore, any binding of [^64^Cu]-NOTA-TRC105-800CW in the tumor would be to the endothelial cells rather than to the tumor cells. Mice bearing 4T1 cell tumors (n = 3 animals/time point) were intravenously injected with 5–10 MBq (135–270 μCi; 300 pmol); the final concentration of [^64^Cu]-NOTA-TRC105-800CW or [^64^Cu]-NOTA-cetuximab-800CW used for the injections was adjusted with unlabeled NOTA-TRC105-800CW or NOTA-cetuximab-800CW (11). Five-minute PET scans were acquired from the animals at predetermined time points (4, 24, and 48 h postinjection (p.i.)), and the region-of-interest (ROI) analysis of each scan was performed with appropriate software to calculate the percentage of injected dose per gram of tissue (% ID/g). The tumors were faintly visible in the images at 4 h p.i. and were clearly distinguishable from the surrounding tissues at 24 h p.i. and 48 h p.i. The amount of radioactivity from [^64^Cu]-NOTA-TRC105-800CW in the blood, liver, and tumor at the different time points is shown in Table 1.

Table 1: Amount of radioactivity from [ ^ 64 ^ Cu]-NOTA-TRC105-800CW in various tissues of mice bearing 4T1 cell tumors at the different time points ( 11 ).

Tissue | % ID/g at various time points p.i.
Tissue | 4 h | 24 h | 48 h
Blood | 19.6 ± 3.0 (21.3 ± 2.5) | 11.4 ± 1.8 (11.2 ± 1.3) | 9.4 ± 0.4 (7.6 ± 0.4)
Liver | 16.4 ± 3.1 (17.5 ± 2.5) | 10.8 ± 1.1 (11.3 ± 1.6) | 11.7 ± 4.4 (11.4 ± 1.1)
Tumor | 5.2 ± 2.7 (~2.5)# | 11.0 ± 1.4 (~4.0)#* | 13.0 ± 0.4 (~5.0)#*

# Values derived from time-activity curves; *P < 0.01.

Numbers in parenthesis represent radioactivity accumulated in the tissues of animals (n = 3 mice/time point) pretreated with a blocking dose (~15 nmol) of unlabeled TRC105 2 h before the [ ^ 64 ^ Cu]-NOTA-TRC105-800CW injection.

For the blocking study, the animals were injected with ~15 nmol unlabeled TRC105 2 h before administration of [^64^Cu]-NOTA-TRC105-800CW (11). At all the time points, the uptake of radioactivity in the blood, liver, and tumors from [^64^Cu]-NOTA-cetuximab-800CW (used as a negative control) was significantly less than that from [^64^Cu]-NOTA-TRC105-800CW (P < 0.05 at 4 h p.i.; P < 0.01 at 24 h and 48 h p.i.). Results obtained from this study indicated that the ^64^Cu- and NIRF-labeled TRC105 mAb had a high binding specificity for the CD105 antigen in vivo.

NIRF images of the animals (n = 3 mice/time point) were acquired immediately after the PET scans at the same time points as mentioned above (11). The tumor fluorescence signal intensity was 7.11 × 10^4^ ± 0.86 × 10^4^ counts/s/ mm^2^, 1.56 × 10^5^ ± 1.54 × 10^4^ counts/s/mm^2^, and 1.19 × 10^5^ ± 2.41 × 10^4^ counts/s/mm^2^ at 4, 24, and 48 h p.i., respectively. The fluorescence intensity of tumors from animals pretreated with unlabeled TRC105 was significantly reduced (4.04 × 10^4^ ± 1.20 × 10^4^ counts/s/mm^2^, 8.97 × 10^4^ ± 0.66 × 10^4^ counts/s/mm^2^, and 7.75 × 10^4^ ± 1.36 × 10^4^ counts/s/mm^2^ at 4, 24, and 48 h p.i., respectively; P < 0.05 at 24 h and 48 h p.i. compared to animals injected with [^64^Cu]-NOTA-TRC105-800CW alone). These results were similar to those obtained from the PET study and indicated that [^64^Cu]-NOTA-TRC105-800CW had an in vivo binding specificity for the CD105 antigen.

Results obtained from ex vivo PET and NIRF images of the major organs harvested from the animals were similar to those obtained with whole-body PET and NIRF imaging (11). The ex vivo images showed that tumors from mice injected with [^64^Cu]-NOTA-TRC105-800CW had a very high contrast compared with the contrast of tumors from animals injected with a blocking dose of either unlabeled TRC105 or [^64^Cu]-NOTA-cetuximab-800CW. The NIRF signal intensities of the in vivo and the ex vivo tumors were similar at 48 h p.i. (1.19 × 10^5^ ± 2.41 × 10^4^ counts/s/mm^2^versus 1.31 × 10^5^ ± 1.58 × 10^4^ counts/s/mm^2^) and had a linear correlation R^2^ value of 0.74.

Biodistribution data obtained at 48 h p.i. from different tissues of the mice showed that the tumors had the maximum accumulation of radioactivity from [^64^Cu]-NOTA-TRC105-800CW (~12.5% ID/g) compared with ~10.0%ID/g, ~6.0% ID/g, and ~6.5% ID/g in the liver, lungs, and kidneys, respectively (11). In addition, a significantly decreased (P < 0.05) uptake of radioactivity was observed in the tumors of mice pretreated with a blocking dose of unlabeled TRC105 (~4.0% ID/g) or in tumors of mice injected with [^64^Cu]-NOTA-cetuximab-800CW (~4.5% ID/g).

Frozen tumor sections were treated with TRC105 and an anti-CD31 antibody (the CD31antigen is an endothelial biomarker) followed by exposure to appropriate secondary antibodies to visualize the expression of CD105 and CD31 in the lesions (11). Fluorescence microscopy of the immunostained sections showed that there was co-localization of the CD105 and CD31 stains in the frozen sections, indicating that TRC105 bound only to the endothelial cells. In addition, CD105 was expressed only on actively proliferating endothelial cells of the tumor, which are located toward the periphery of the tumor (compared with the center of the lesion) where angiogenesis is most active. Mature blood vessels showed a very low expression of CD105.

From these studies, the investigators concluded that PET/NIRF agents can be used for the detection of tumors in rodents (11).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-TRC105-800CW%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-TRC105-800CW%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B64Cu%5D-NOTA-TRC105-800CW%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

This work was supported, in part, by the National Institutes of Health through the UW Radiological Sciences Training Program 5 T32 CA009206-32.

## References

1 Nassiri F., Cusimano M.D., Scheithauer B.W., Rotondo F., Fazio A., Yousef G.M., Syro L.V., Kovacs K., Lloyd R.V. (2011). Endoglin (CD105): a review of its role in angiogenesis and tumor diagnosis, progression and therapy. Anticancer Res.
2 Perez-Gomez E., Del Castillo G., Juan Francisco S., Lopez-Novoa J.M., Bernabeu C., Quintanilla M. (2010). The role of the TGF-beta coreceptor endoglin in cancer. ScientificWorldJournal.
3 Fonsatti E., Nicolay H.J., Altomonte M., Covre A., Maio M. (2010). Targeting cancer vasculature via endoglin/CD105: a novel antibody-based diagnostic and therapeutic strategy in solid tumours. Cardiovasc Res.
4 Seon B.K., Haba A., Matsuno F., Takahashi N., Tsujie M., She X., Harada N., Uneda S., Tsujie T., Toi H., Tsai H., Haruta Y. (2011). Endoglin-targeted cancer therapy. Curr Drug Deliv.
5 Shiozaki K., Harada N., Greco W.R., Haba A., Uneda S., Tsai H., Seon B.K. (2006). Antiangiogenic chimeric anti-endoglin (CD105) antibody: pharmacokinetics and immunogenicity in nonhuman primates and effects of doxorubicin. Cancer Immunol Immunother.
6 Hong H., Yang Y., Zhang Y., Engle J.W., Barnhart T.E., Nickles R.J., Leigh B.R., Cai W. (2011). Positron emission tomography imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
7 Hong H., Severin G.W., Yang Y., Engle J.W., Zhang Y., Barnhart T.E., Liu G., Leigh B.R., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of CD105 expression with 89Zr-Df-TRC105. Eur J Nucl Med Mol Imaging.
8 Yang Y., Zhang Y., Hong H., Liu G., Leigh B.R., Cai W. (2011). In vivo near-infrared fluorescence imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
9 Kobayashi H., Longmire M.R., Ogawa M., Choyke P.L. (2011). Rational chemical design of the next generation of molecular imaging probes based on physics and biology: mixing modalities, colors and signals. Chem Soc Rev.
10 Thorp-Greenwood F.L., Coogan M.P. (2011). Multimodal radio- (PET/SPECT) and fluorescence imaging agents based on metallo-radioisotopes: current applications and prospects for development of new agents. Dalton Trans.
11 Zhang Y., Hong H., Engle J.W., Yang Y., Theuer C.P., Barnhart T.E., Cai W. (2012). Positron Emission Tomography and Optical Imaging of Tumor CD105 Expression with a Dual-Labeled Monoclonal Antibody. Mol Pharm.